# ^68^Ga-Labeled anti-EpCAM diabody against epithelial cell adhesion molecule

Chemical name: | ^68^Ga-Labeled anti-EpCAM diabody against epithelial cell adhesion molecule
Abbreviated name: | ^68^Ga-HBED-CC-anti-EpCAM diabody
Synonym:
Agent category: | Affibody, antibody fragment
Target: | Epithelial cell adhesion molecule (EpCAM)
Target category: | Adhesion molecule
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/NP_002345.2), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_002354.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=4072) for more information about EpCAM.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM)]

Epithelial cell adhesion molecules (EpCAM) are found on the cell surface of epithelial cells of many epithelial tissues such as the pancreas, jejunum, colon, kidney, salivary gland, and prostate (1). EpCAM is responsible for intracellular signaling and polarity, and it mediates cell differentiation, proliferation, migration, and adhesion (2, 3). It is a pan-epithelial (http://en.wikipedia.org/wiki/Epithelial) differentiation antigen (http://en.wikipedia.org/wiki/Antigen) that is expressed on almost all carcinomas (http://en.wikipedia.org/wiki/Carcinomas) (4). Approximately 70% of human prostate cancers show high levels of EpCAM expression (5, 6).

Single-chain variable fragments (scFvs) of antibodies with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (7). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass, 55 kDa) has been evaluated for targeting in several tumor antigen systems and has demonstrated rapid tumor localization and high-contrast imaging (7, 8). In particular, human IgG^42^ anti-EpCAM (clone 42 (huIgG^42^), ~150kDa) was isolated from a human naïve antibody library. The monomeric scFv^42^_18_ (clone 42 with 18 amino acid linker), dimeric scFv^42^_9_ (diabody), and trimeric scFv^42^_0_ (tribody) were genetically constructed. These fragments retain excellent EpCAM-binding properties (dissociation constant (K_d_) = 0.24–11.8 nM) and were developed as EpCAM imaging agents. They were conjugated with the bifunctional chelating agent N,N'-bis[2-hydroxy-5-(carboxyethyl)benzyl]ethylenediamine-N,N'-diacetic acid (HBED-CC) to enable labeling with ^68^Ga for imaging of EpCAM expression in solid tumors (9).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EpCAM+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (EpCAM (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4072))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/185535)
- Clinical trials (EpCAM (http://www.clinicaltrials.gov/ct2/results?term=EpCAM))
- Drug information in FDA (EpCAM (http://google2.fda.gov/search?q=EpCAM&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM%20and%20synthesis)]

All antibody variants were conjugated with HBED-CC with ~1 HBED-CC per antibody molecule (9). The conjugates were incubated with ^68^Ga^3+^ for 5 min at pH 4.2 at room temperature. Radiochemical yields were >90% with specific activities of 20–36 GBq/µmol (0.7–1.0 Ci/µmol) for all variants at the end of purification. ^68^Ga-HBED-CC-scFv^42^_18_, ^68^Ga-HBED-CC-diabody, ^68^Ga-HBED-CC-tribody, and ^68^Ga-HBED-CC-huIgG^42^ were stable in 50% human serum for 4 h at 37ºC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM%20and%20in%20vitro)]

Eder et al. (9) performed binding experiments with the antibody variants using a Biacore sensor chip immobilized with EpCAM-Fc. The K_d_ values were 11.8, 0.24, and 0.29 for scFv^42^_18_, dimeric scFv^42^_9_ (diabody), and trimeric scFv^42^_0_ (tribody), respectively. Binding specificity tests in vitro showed that binding of ^68^Ga-labeled antibody variants to HT-29 cells expressing EpCAM was receptor-mediated because saturation of receptors by preincubation with a non-labeled antibody variant significantly decreased binding of the corresponding antibody variant. The 50% inhibition concentrations were 58.8, 9.2, 4.8, and 6.7 nM for scFv^42^_18_, diabody, tribody, and huIgG^42^, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM%20and%20rodentia)]

Eder et al. (9) performed ex vivo biodistribution studies of ^68^Ga-HBED-CC-scFv^42^_18_, ^68^Ga-HBED-CC-diabody, ^68^Ga-HBED-CC-tribody, and ^68^Ga-HBED-CC-huIgG^42^ in nude mice (n = 3/group) bearing HT-29 xenografts after injection of 1–2 MBq (0.027–0.54 mCi) per mouse. The tumor radioactivity was 0.62%, 1.87%, 3.01%, and 3.54% injected dose/gram (ID/g), respectively, at 1 h after injection. There was a rapid renal clearance from blood for the antibody variants. The diabody exhibited the highest kidney radioactivity of 122% ID/g at 1 h. The radioactivity level of the diabody in the blood, lung, heart, intestine, spleen, muscle, and bone was low (<3% ID/g) at 2–3 h after injection. The full-length antibody and tribody revealed high radioactivity levels in the blood, lung, liver, kidney, heart, and spleen at 1-3 h. The diabody showed the best tumor/blood ratio of ~2 at 3 h after injection. In another experiment, tumor accumulation of ^68^Ga-HBED-CC-diabody was performed in nude mice (n = 3) bearing HT-29 (high EpCAM expression) and LoVo (low EpCAM expression) xenografts. The accumulation in the HT-29 tumor (1.87 ± 0.50% ID/g) was significantly higher (P < 0.05) than the accumulation in the LoVo tumor (0.80 ± 0.40% ID/g). PET imaging was performed in nude mice bearing A-431 tumors. The tumors and kidneys were clearly visualized at 1 h after injection of ^68^Ga-HBED-CC-diabody. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20EpCAM%20and%20human)]

No publication is currently available.

## References

1 Trzpis M., McLaughlin P.M., de Leij L.M., Harmsen M.C. (2007). Epithelial cell adhesion molecule: more than a carcinoma marker and adhesion molecule. Am J Pathol.
2 Balzar M., Prins F.A., Bakker H.A., Fleuren G.J., Warnaar S.O., Litvinov S.V. (1999). The structural analysis of adhesions mediated by Ep-CAM. Exp Cell Res.
3 Balzar M., Winter M.J., de Boer C.J., Litvinov S.V. (1999). The biology of the 17-1A antigen (Ep-CAM). J Mol Med.
4 Armstrong A., Eck S.L. (2003). EpCAM: A new therapeutic target for an old cancer antigen. Cancer Biol Ther.
5 Poczatek R.B., Myers R.B., Manne U., Oelschlager D.K., Weiss H.L., Bostwick D.G., Grizzle W.E. (1999). Ep-Cam levels in prostatic adenocarcinoma and prostatic intraepithelial neoplasia. J Urol.
6 Went P.T., Lugli A., Meier S., Bundi M., Mirlacher M., Sauter G., Dirnhofer S. (2004). Frequent EpCam protein expression in human carcinomas. Hum Pathol.
7 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
8 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
9 Eder M., Knackmuss S., Le Gall F., Reusch U., Rybin V., Little M., Haberkorn U., Mier W., Eisenhut M. (2010). 68Ga-labelled recombinant antibody variants for immuno-PET imaging of solid tumours. Eur J Nucl Med Mol Imaging.